# Au_3_Cu_1_ Nanoparticles

Chemical name: | Au_3_Cu_1_ Nanoparticles
Abbreviated name: | Au_3_Cu_1_-NPs
Synonym:
Agent Category: | Metal
Target: | Non-targeted
Target Category: | Blood-pool retention
Method of detection: | MRI
Source of signal\contrast: | Cu
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=gold+nanoshells)]

Magnetic resonance imaging (MRI) maps information about tissues spatially and functionally. Protons (hydrogen nuclei) are widely used in MRI because of their abundance in water molecules. Water comprises ~80% of most soft tissue. The contrast of proton MRI depends largely on the density of the nucleus (proton spins), the relaxation times of the nuclear magnetization (T_1_, longitudinal, and T_2_, transverse), the magnetic environment of the tissues, and the blood flow to the tissues. Insufficient contrast between normal and diseased tissues requires the development of contrast agents. Most contrast agents affect the T_1_ and T_2_ relaxation times of the surrounding nuclei, mainly the protons of water. T_2_* is the spin–spin relaxation time composed of variations from molecular interactions and intrinsic magnetic heterogeneities of tissues in the magnetic field (1). Cross-linked iron oxide nanoparticles and other iron oxide formulations primarily affect T_2_ and lead to decreased signals. On the other hand, paramagnetic T_1_ agents such as gadolinium (Gd^3+^) and manganese (Mn^2+^) accelerate T_1_ relaxation and lead to brighter contrast images (2).

Gold nanoparticles have been used as X-ray and optical contrast agents in small animals with little toxicity (3). Su et al. (4) have developed hollow Au_3_Cu_1_ nanoparticles (nanoshells and nanocapsules) as bimetallic MRI contrast agents with enhancing effects in T_1_- and T_2_-weighted imaging. A Cu^3+^ ion has an electron configuration of d^8^ with two unpaired electrons and less magnetic moment than Gd^3+^, with seven unpaired electrons; however, hollow Au_3_Cu_1_ nanoparticles are made of large numbers of paramagnetic Cu^3+^ ions to provide a superparamagnetic effect. The large surface area of the porous nanoparticles also provides an effective interaction of Cu^3+^ ions with water molecules.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=gold+nanoshells+synthesis)]

Su et al. (4) produced Au_3_Cu_1_ nanoparticles by adding 1 × 10^-6^ mol HAuCl_4_ (dehydrated) to a Cu-colloidal solution, which was prepared with laser irradiation of CuO in 2-propanol. The mixture was sonicated for 10 min to form hollow Au_3_Cu_1_ nanoshells. The Au_3_Cu_1_ nanoshells were coated with polyelectrolyte polyethylenimine (PEI) and poly(acrylic acid) (PAA) polymers to form Au_3_Cu_1_ nanocapsules. The nanoshell cores were 48.9 ± 19.1 nm in diameter, and the shells were 5.8 ± 1.8 nm thick as determined with transmission electron microscopy. The pores were 1–2 nm in diameter. The nanocapsule shells were 6.1 ± 1.2 nm thick. The number of copper atoms/nanoparticle was estimated to be 4.98 × 10^5^.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=gold+nanoshells+in+vitro)]

For in vitro MR images as well as both T_1_ and T_2_ measurements at 3 T, all nanoshells and nanocapsules were dispersed in 5% agarose gel at various concentrations (0.125, 0.25, 1.25, 2.5, and 5 mg/ml) (4). Adding Au_3_Cu_1_ nanocapsules to the agarose gel brightened the T_1_ image and enhanced the T_1_^-1^ (longitudinal relaxation rate) of water protons. The T_1_-weighted MR signal intensity increased up to ~89% as the Au_3_Cu_1_ nanocapsule concentrations increased from 0 to 5.00 mg/mL; however, use of Au_3_Cu_1_ nanoshells resulted in only ~26% increase in T_1_ image intensity. Interestingly, both nanoparticles enhanced T_2_-weighted image intensity by 8% to 11% at 0.125 mg/ml and decreased by 6% and 76% at 5 mg/ml for nanoshells and nanocapsules, respectively. The proton r_1_ relaxivities were as large as 3.0 × 10^4^ mM^-1^s^-1^ (Au_3_Cu_1_ nanocapsules) and 2.3 × 10^4^ mM^-1^s^-1^ (Au_3_Cu_1_ nanoshells). The proton r_2_ relaxivities were 2.39 × 10^5^ mM^-1^s^-1^ for Au_3_Cu_1_ nanocapsules and 1.82 × 10^6^ mM^-1^s^-1^ for Au_3_Cu_1_ nanoshells. Both exhibited little cytotoxicity to monkey kidney epithelial Vero cells in culture at concentrations of 0.1–10,000 ng/ml at 37°C up to 24 h.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=gold+nanoshells+%20rodentia)]

Su et al. (4) studied the long-term toxicological effects in normal mice (n = 6 mice/group) at 30 days after intravenous injection of 2, 20, and 40 mg/kg Au_3_Cu_1_ nanocapsules with viability rates of 100%, 83%, and 67%, respectively. Most of the Au and Cu were found in the urine at 3 h after injection. MRI studies (T_1_- and T_2_-weighted imaging at 3 T) were performed in normal mice after injection of 20 mg/kg Au_3_Cu_1_ nanocapsules. Both images were enhanced in the heart and major vessels at 2 h after injection. Images of the blood vessels in the liver were also enhanced. The calculated blood concentration is ~0.25mg/ml after injection of 20 mg/kg. Au_3_Cu_1_ nanocapsules may be a tool as positive contrast agent for use in MR angiography.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=gold+nanoshells+and%20%28pig%20or%20dog%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=gold+nanoshells+and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=gold+nanoshells+human)]

No publication is currently available.

## References

1 Wang Y.X., Hussain S.M., Krestin G.P. (2001). Superparamagnetic iron oxide contrast agents: physicochemical characteristics and applications in MR imaging. Eur Radiol.
2 Kabalka G., Buonocore E., Hubner K., Moss T., Norley N., Huang L. (1987). Gadolinium-labeled liposomes: targeted MR contrast agents for the liver and spleen. Radiology.
3 Hainfeld J.F., Slatkin D.N., Focella T.M., Smilowitz H.M. (2006). Gold nanoparticles: a new X-ray contrast agent. Br J Radiol.
4 Su C.H., Sheu H.S., Lin C.Y., Huang C.C., Lo Y.W., Pu Y.C., Weng J.C., Shieh D.B., Chen J.H., Yeh C.S. (2007). Nanoshell magnetic resonance imaging contrast agents. J Am Chem Soc.